# ^186^Re-Labeled [N-[2-[[4-[(4-hydroxy-4,4-diphosphonobutyl)amino]-4-oxobutyl]-2-thioethylamino]acetyl]-2-aminoethanethiolate] oxorhenium (V)

Chemical name: | ^186^Re-Labeled [N-[2-[[4-[(4-hydroxy-4,4-diphosphonobutyl)amino]-4-oxobutyl]-2-thioethylamino]acetyl]-2-aminoethanethiolate] oxorhenium (V)
Abbreviated name: | [^186^Re]MAMA-HBP
Synonym:
Agent Category: | Compound
Target: | Hydroxyapatite: Bone imaging Molecular target: Farnesyl disphosphate (pyrophosphate) synthase
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^186^Re
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^186^Re]MAMA-HBP for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipycolylamine%20alendronate&cmd=DetailsSearch)]

Bisphosphonates (BPs) or nitrogen-containing bisphosphonates (NBPs) are often used for the management of pain palliation and disorders related to skeletal tissue, including those arising from cancer metastases, because these compounds have a very high affinity for hydroxyapatite (HA), a component of the bone matrix. These phosphonates or their derivatives tend to accumulate in osteoclasts located at areas of increased bone metabolism by inhibiting the enzyme farnesyl diphosphate (or pyrophosphate) synthase, an important enzyme of the cellular mevalonate pathway, which is involved in protein prenylation (1). The mechanism of action of BPs and the NBPs has been described in detail by Drake et. al. (2). Several BPs and NBPs are commercially available for clinical use to treat different bone disorders, and there are ongoing clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) approved by the United States Food and Drug Administration to evaluate these compounds for the treatment of various bone ailments. In addition, BPs are often labeled with ^99m^Tc or ^186/188^Re and used for the imaging and treatment of pain as a result of bone metastases from cancer such as that of the breast or the prostate (3). However, these compounds have limited efficacy primarily because they exist either as a mixture of anionic compounds with varying properties (e.g., ^99m^Tc-labeled methyl diphosphonate (MDP)) or are unstable (e.g., ^86^Re-labeled 1-hydroxyethylidene-1,1-diphosphonate) under in vivo conditions, resulting in a reduced uptake at targeted bone areas and an increased accumulation in non-target soft tissue such as the gastric lining of the stomach (4). The limited clinical utility of radiolabeled BPs was suggested to be caused by the dual activities exhibited by the compounds: one phosphonate group acts as a radionuclide chelator, and the other phosphonate group binds to the target(s). Therefore, due to the close proximity of the two groups, one activity may be interfering with the other (4).

In an effort to solve the stability problems observed with the ^186^Re-labeled NBPs, Ogawa et al. developed two new NBPs, ^186^Re-[N-[2-[[3-(3,3-diphosphonopropylcarbamoyl)propyl]-2-thioethylamino]acetyl]-2-aminoethylenethiolate] oxorhenium (V) ([^186^Re]MAMA-BP) and its hydroxylated derivative, ^186^Re-[N-[2-[[4-[(4-hydroxy-4,4-diphosphonobutyl)amino]-4-oxobutyl]-2-thioethylamino]acetyl]-2-aminoethanethiolate] oxorhenium (V) ([^186^Re]MAMA-HBP) (3). The two compounds were then compared for their affinity to HA under in vitro conditions and the biodistribution of the radiochemicals was investigated in normal mice. This chapter presents the results obtained with [^186^Re]MAMA-HBP. Results obtained with [^186^Re]MAMA-BP are presented in a separate chapter of MICAD (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonate%20synthesis&cmd=DetailsSearch)]

The synthesis of [^186^Re]MAMA-HBP was done as described by Ogawa et al. (3). The radiochemical yield and purity of [^186^Re]MAMA-HBP were reported to be 54% and >95%, respectively. The synthesis of [^186^Re]MAMA-BP (for comparative studies) and ^186^Re-1-hydroxyethylidene-1,1-diphosphonate ([^186^Re]MAMA-HEDP; used as a control in the various studies) is detailed elsewhere (6). Specific activity of the radiolabeled compounds was not reported. The in vitro stability of [^186^Re]MAMA-HBP after a 24-h incubation in 0.1 M phosphate-buffered saline (pH, 7.0) saturated with 95% O_2_ and 5% CO_2_ at 37°C was reported to be 75.55 ± 1.57% as determined with reversed-phase high-performance liquid chromatography or thin-layer chromatography. In an earlier study, the stability of [^186^Re]MAMA-BP was reported to be 81.8 ± 1.7% under the same conditions (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonate%20in%20vitro%20stability&cmd=DetailsSearch)]

The HA binding of [^186^Re]MAMA-HBP was determined by using different amounts (1–25 mg/mL) of commercially available HA beads suspended in Tris/HCl-buffered saline (pH, 7.4) as described by Ogawa et al. (3). The percent of HA binding was determined with an equation given elsewhere (3). Approximately 70% of [^186^Re]MAMA-HBP bound to the HA beads at the lowest concentration (compared with ~40% for [^186^Re]MAMA-BP) and increased to ~97.5% at the highest concentration (compared with ~95.0% for [^186^Re]MAMA-BP). Results from this study indicated that [^186^Re]MAMA-HBP had a higher affinity for HA than [^186^Re]MAMA-BP. In another study, increasing concentrations of unlabeled HEDP were shown to significantly (P < 0.05) reduce the HA binding of [^186^Re]MAMA-HBP.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonate%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^186^Re]MAMA-HBP, [^186^Re]MAMA-BP, and [^186^Re]MAMA-HEDP (control) was investigated in normal, male ddY mice after intravenous administration of the respective labeled compounds (3). The animals (n = 5–6 mice per time point) were euthanized at designated time points ranging from 10 min to 24 h postinjection (p.i.). Organs of interest (liver, kidney, blood, intestine, stomach, and the complete left femur) were removed from the cadavers and weighed, and the amount of radioactivity accumulated in the tissues was measured, and the data were presented as percent injected dose per gram tissue (% ID/g).

The tissue distribution pattern of radioactivity from [^186^Re]MAMA-HBP was reported to be similar to that observed with [^186^Re]MAMA-BP and [^186^Re]MAMA-HEDP (3). Maximum label was deposited on the femur at all time points with the three radiochemicals (24.80 ± 2.41% ID/g with [^186^Re]MAMA-HBP, 21.38 ± 3.83% ID/g with [^186^Re]MAMA-BP, and 13.09 ± 2.90% ID/g with [^186^Re]MAMA-HEDP) at 24 h p.i., followed by the kidneys (varying from 0.42 ± 0.10% ID/g with [^186^Re]MAMA-HEDP, 0.87 ± 0.24% ID/g with [^186^Re]MAMA-HBP, and 2.43 ± 0.53% ID/g with [^186^Re]MAMA-BP) at the same time point. The femur/blood ratios of accumulated radioactivity were ~1,200 with [^186^Re]MAMA-HBP compared with ~800 and ~400 with [^186^Re]MAMA-BP and [^186^Re]MAMA-HEDP, respectively. In addition, the blood clearance of radioactivity from [^186^Re]MAMA-HEDP was slower than that of the other two ^186^Re-labeled MAMA-bisphosphonates, and it had a lower accumulation in the liver.

Ogawa et al. calculated the radiation dose estimates for the three bisphosphonates for adult patients by monoexponential extrapolation of the biodistribution data (3). Although the red-marrow/bone-surface and total-body/bone-surface ratios for all the radiolabeled compounds were the same, the effective-dose/bone-surface ratio of [^186^Re]MAMA-HEDP was higher than that of either [^186^Re]MAMA-BP or [^186^Re]MAMA-HBP.

From these studies, the investigators concluded that [^186^Re]MAMA-HBP has a higher affinity for the bone than either [^186^Re]MAMA-BP or [^186^Re]MAMA-HEDP (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonates%20non%20primate%20mammal%20studies&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nitrogen%20containing%20bisphosphonates%20non%20human%20primate%20studies&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
2 Drake M.T., Clarke B.L., Khosla S. (2008). Bisphosphonates: mechanism of action and role in clinical practice. Mayo Clin Proc.
3 Ogawa K., Mukai T., Arano Y., Otaka A., Ueda M., Uehara T., Magata Y., Hashimoto K., Saji H. (2006). Rhemium-186-monoaminemonoamidedithiol-conjugated bisphosphonate derivatives for bone pain palliation. Nucl Med Biol.
4 Torres Martin de Rosales R., Finucane C., Mather S.J., Blower P.J. (2009). Bifunctional bisphosphonate complexes for the diagnosis and therapy of bone metastases. Chem Commun (Camb).
5 Chopra, A., 186Re-Labeled [N-[2[[3-[(3,3-diphosphonopropylcarbamoyl)propyl]-2-thioethylamino]acetyl]-2-aminoethanethiolate] oxorhenium (V). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
6 Ogawa K., Mukai T., Arano Y., Hanaoka H., Hashimoto K., Nishimura H., Saji H. (2004). Design of a radiopharmaceutical for the pallation of painful bone metastases: rhenium-186-labeled bisphosphonate derivative. J. Label. Compd. Radiopharm.